# Cy5.5-Knottin 2.5F

Chemical name: | Cy5.5-Knottin 2.5F
Abbreviated name: | Cy5.5-Knottin 2.5F
Synonym:
Agent Category: | Ligand
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptors
Method of detection: | Near-infrared fluorescence
Source of signal / contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrin receptors that mediate tumor angiogenesis, growth, and metastasis through a complex network of signaling pathways are known to be expressed on the surface of cancerous tumor cells and neovasculature (1-3). Because of their role in tumor development and progression, inhibition of integrin receptor activity is being actively investigated in clinical trials for the treatment (http://clinicaltrials.gov/ct2/results?term=integrin+inhibitors) and imaging (http://clinicaltrials.gov/ct2/results?term=integrin+imaging) of various cancers (4, 5). Non-invasive imaging probes can be used to determine not only the efficacy of integrin-targeted anti-cancer drugs, but also to monitor disease progression and metastasis (6, 7). Although integrin receptors usually bind through the arginine-glycine-aspartic acid (RGD) motif of the extracellular matrix protein ligands, it is the amino acid residues surrounding the RGD motif that determine the receptor specificity and affinity for the ligand (4, 8, 9). As a result of the small size of the drugs, mainly peptides, that target the integrin receptor, it has been challenging to generate peptides containing the RGD motif that have an improved pharmacokinetic behavior, receptor affinity, and tumor uptake for in vivo imaging purposes. Any modification of the peptide structure has yielded integrin-targeted imaging agents that have only a limited advancement and application in the clinics (10, 11). Only one imaging compound with an RGD motif, a radioactive fluorine-labeled cyclic pentapeptide ([^18^F]-galacto-RGD), was determined to be suitable to identify integrin-positive tumors and to investigate α_v_β_3_ integrin expression in humans. However, [^18^F]-galacto-RGD has been shown to have a low tumor uptake, and it generated a high background signal due to accumulation in the liver (12, 13).

In an effort to develop imaging agents for the detection of integrin receptors expressed on tumor cell surface and neovasculature, Kimura et al. (14) used the directed evolution technique (15, 16) to place the integrin-binding RGD motif into a cystine knot peptide (also known as knottins) trypsin inhibitor of the squash plant (Ecballium elaterium) (17). The peptide was reported to have a high affinity for the α_v_β_3_ and α_v_β_5_ or the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors. In general, knottins have a core structure containing a disulfide bond, are resistant to proteolysis, have a high thermodynamic stability, and are nonimmunogenic (14). The knottin peptide containing an RGD motif (designated as knottin 2.5F) was labeled with a near-infrared (NIR) fluorescent cyanine dye, Cy5.5, to obtain Cy5.5-knottin 2.5F, and the Cy5.5 conjugate was used to image integrin-expressing xenograft tumors in mice with NIR fluorescence imaging. It is pertinent to mention that the knottin 2.5F discussed in this chapter and the knottin 2.5D peptide discussed separately in MICAD (www.micad.nih.gov) were developed and investigated by Kimura et al. (14). The structural and amino acid sequence similarities and differences of the two peptides are described elsewhere (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+synthesis)]

The synthesis of knottin 2.5F was performed with the use of the 9-fluorenylmethylcarbonyl-based solid-phase technique as described by Kimura et al. (14). In addition, two other knottin peptides, FN-RGD2 (for use as positive a control) and FN-RDG2 (negative control) were synthesized using the same technique mentioned above. A third peptide, c(RGDyK), was obtained from commercial sources for use as a second control. The amino acid sequence, structure, and properties of the various integrin-binding peptides used for studies described in this chapter are discussed by Kimura et al. (14).

To conjugate knottin 2.5F to Cy5.5, the knottin was mixed with a solution of Cy5.5-N-hydroxysuccinimide ester in dimethylsulfoxide and triethylamine. The reaction was allowed to proceed at room temperature in the dark (duration not reported) with constant monitoring with reverse-phase high-performance liquid chromatography (RP-HPLC) on a C_18_ column (14). Upon completion of the reaction, the conjugated peptide was purified with semi-preparative RP-HPLC and freeze-dried for storage (conditions not reported). The peptide purity and molecular mass were respectively confirmed with analytical RP-HPLC and electrospray or matrix-assisted laser desorption/ionization time-of-flight mass spectrometery. Yield of the final product, the number of Cy5.5 molecules conjugated to each molecule of knottin 2.5F, and the stability of the fluorescent dye–labeled knottin were not reported.

Echistatin labeled with radioactive iodine (^125^I-echistatin), used as a control in some studies, was obtained from a commercial source (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy55+knottin+2%2E5D+in+vitro)]

To determine the relative integrin-binding affinities (reported as 50% inhibitory concentration (IC_50_)) of the modified and unmodified peptides, including knottin 2.5F, a competition binding assay was performed with ^125^I-echistatin (a strong antagonist of α_v_β_3_, α_v_β_5_, α_5_β_1_ and α_iib_β_3_ integrins (14)) using U-87MG cells (a human glioblastoma cell line that expresses several types of integrins on the cell surface) as described by Kimura et al. (14). The IC_50_ for Cy5.5-knottin 2.5F was determined to be 3.5 ± 0.8 nmol/L compared with IC_50_ values of 26.5 ± 5.0 nmol/L, 370 ± 150 nmol/L, and 860 ± 400 nmol/L for the unconjugated knottin 2.5F, control FN-RGD2 and c(RGDyK) peptides, respectively. The negative control FN-RDG2 peptide, with or without Cy5.5 conjugation, did not compete with ^125^I-echistatin for binding to the U-87MG cells (14).

The integrin-binding specificity of Cy5.5-knottin 2.5F was investigated with a competition displacement assay using immobilized integrin receptors and ^125^I-echistatin (14). Different concentrations (5 and 50 nmol/L) of the conjugated knottin 2.5F and the control peptides were respectively incubated with ^125^I-echistatin in microtiter plates coated with detergent-solubalized α_v_β_3_, α_v_β_5_, α_5_β_1_, and α_iib_β_3_ integrin receptors for 3 h at room temperature. The plates were washed three times to remove unbound radioactivity, and the contents were solubalized in 2 N sodium hydroxide to determine the amount of receptor-bound radioactivity. Compared with the conjugated FN-RGD2 and c(RGDyK) peptides, the Cy5.5-knottin 2.5F peptide exhibited a high competition for^125^I-echistatin binding to the different integrin receptors (varying from ~35 to 95% reduction in binding of labeled echistatin using a low (5nmol/L) and a high (50 nmol/L) concentration of the unlabeled peptides) except the α_iib_β_3_ receptor, which is expressed mainly on blood platelet cells (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy55+knottin+2%2E5D+rodentia)]

The use of Cy5.5-knottin 2.5F as an NIR imaging probe was investigated in mice bearing human U-87MG cell xenograft tumors and compared with imaging results obtained with the Cy5.5-conjugated control peptides (14). The animals (n = 3 mice for each probe) were injected with the respective Cy5.5-conjugated peptides through the tail vein and imaged at various time points up to 24 h. Whole-body imaging was performed on the animals, and the tumor/normal tissue fluorescence ratios (T/N) were calculated. The T/N ratios generated (for details see Figure 3B in reference 14) with Cy5.5-knottin 2.5F had a low standard deviation (~3.0 at 1 h and ~3.75 at 24 h) and were significantly (P < 0.05) higher than those obtained from the control Cy5.5-conjugated peptides (~2.2 at 1 h and ~3.0 at 24 h) at all time points from 0 to 24 h after administration of the probes. Also, the signal obtained with the positive control Cy5.5-conjugated peptides was only slightly higher than that of the negative control, FN-RDG2 peptide (~2 at 1 h and 2.5 at 24 h). No in vivo biodistribution of the Cy5.5-conjugated knottin 2.5F peptide was reported.

From these studies the investigators concluded that the direct evolution–engineered integrin-binding peptides are probably suitable for the detection and diagnosis of various cancers (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy55+knottin+2%2E5D+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy55+knottin+2%2E5D+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5%2E5+knottin+2%2E5D+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the work presented in this chapter was supported by National Cancer Institute grants 5K01 CA104706, 5R25T CA118681, and R25T CA118681 and a National Institutes of Health grant P50 CA114747.

## References

1 Legate K.R., Wickstrom S.A., Fassler R. (2009). Genetic and cell biological analysis of integrin outside-in signaling. Genes Dev.
2 Pontier S.M., Muller W.J. (2009). Integrins in mammary-stem-cell biology and breast-cancer progression--a role in cancer stem cells?. J Cell Sci.
3 Streuli C.H. (2009). Integrins and cell-fate determination. J Cell Sci.
4 Moschos S.J., Drogowski L.M., Reppert S.L., Kirkwood J.M. (2007). Integrins and cancer. Oncology.
5 Fujita Y., Abe R., Shimizu H. (2008). Clinical approaches toward tumor angiogenesis: past, present and future. Curr Pharm Des.
6 Zaccaro L., Del Gatto A., Pedone C., Saviano M. (2009). Peptides for tumour therapy and diagnosis: current status and future directions. Curr Med Chem.
7 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
8 Chen, C.Y., J.H. Shiu, Y.H. Hsieh, Y.C. Liu, Y.C. Chen, Y.C. Chen, W.Y. Jeng, M.J. Tang, S.J. Lo, and W.J. Chuang, Effect of D to E mutation of the RGD motif in rhodostomin on its activity, structure, and dynamics: Importance of the interactions between the D residue and integrin. Proteins, 2009
9 Manzoni, L., L. Belvisi, D. Arosio, M. Civera, M. Pilkington-Miksa, D. Potenza, A. Caprini, E.M. Araldi, E. Monferini, M. Mancino, F. Podesta, and C. Scolastico, Cyclic RGD-Containing Functionalized Azabicycloalkane Peptides as Potent Integrin Antagonists for Tumor Targeting. ChemMedChem, 2009
10 Cai W., Rao J., Gambhir S.S., Chen X. (2006). How molecular imaging is speeding up antiangiogenic drug development. Mol Cancer Ther.
11 Haubner R. (2006). Alphavbeta3-integrin imaging: a new approach to characterise angiogenesis?. Eur J Nucl Med Mol Imaging.
12 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
13 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
14 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
15 Otten L.G., Quax W.J. (2005). Directed evolution: selecting today's biocatalysts. Biomol Eng.
16 Leemhuis H., Kelly R.M., Dijkhuizen L. (2009). Directed evolution of enzymes: Library screening strategies. IUBMB Life.
17 Favel A., Mattras H., Coletti-Previero M.A., Zwilling R., Robinson E.A., Castro B. (1989). Protease inhibitors from Ecballium elaterium seeds. Int J Pept Protein Res.